# Complement receptor type 2–conjugated superparamagnetic iron oxide nanoparticles

Chemical name: | Complement receptor type 2–conjugated gold/superparamagnetic iron oxide nanoparticles
Abbreviated name: | CR2-Fc-SPIO
Synonym:
Agent category: | Receptor
Target: | Complement C3 fragments
Target category: | Protein
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. SPIO nanoparticles are sometimes modified with dextran, poly(ethylene glycol) (PEG), or other biomaterials to reduce RES uptake and to prolong blood half-life. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific molecular imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

The complement system consists of >30 proteins and acts as important part of the innate immune system. Complement activation helps eliminate pathogens during infection but also causes injury to host tissues in autoimmune diseases such as systemic lupus erythematosus (2) and allergic asthma (3). Most lupus patients develop renal abnormalities with glomerular deposition of C3 fragments (C3b, iC3b, and C3d) (4). Complement receptor type 2 (CR2, CD21) binds C3 fragments but does not bind C3 (5). Serkova et al. (6) conjugated a recombinant protein containing the C3d-binding region of CR2 to SPIO nanoparticles. CR2-Fc-SPIO nanoparticles were evaluated in a mouse model of lupus nephritis.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=SPIO+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad) (SPIO)
- Gene information in NCBI (CR2 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=1380))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/120650) (CR2)
- Clinical trials (SPIO (http://www.clinicaltrials.gov/ct2/results?term=Feridex))
- Drug information in FDA (SPIO (http://google2.fda.gov/search?q=Feridex&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20synthesis)]

A recombinant protein containing the C3d-binding region of CR2 was linked to the Fc portion of mouse IgG_1_ (6). The recombinant protein (6.7 µmol) was incubated with SPIO (10 nm in diameter) containing 1.5 nmol Fe, 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide, and N-hydroxysulfosuccinimide for 2 h at room temperature. CR2-Fc-SPIO nanoparticles were purified with high-speed centrifugation. The copies of protein per SPIO were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20in%20vitro)]

Chinese hamster ovary (CHO) cells were incubated with 10% normal mouse serum to opsonize C3 fragments on their cell surface. The binding of serum proteins on the cell surface enhanced phagocytosis of C3 fragments in the serum. Flow cytometry analysis confirmed binding of CR2-Fc-SPIO to the opsonzied CHO cells, whereas SPIO did not bind to the opsonzied CHO cells. Furthermore, CR2-Fc-SPIO did not bind to unopsonized CHO cells. Cy3-Labeled anti-mouse IgG was used to detect CR2-Fc-SPIO.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20rodentia)]

Serkova et al. (6) performed T2-weighted MRI (4.7 T) in MRL/lpr lupus mice (n = 5) and normal wild-type mice (n = 6) with CR2-Fc-SPIO and SPIO (10–16 mg/kg) at 4–72 h after injection. T2 relaxation times in the muscle, fat, and spleen were similar in both groups before injection of nanoparticles. Injection of CR2-Fc-SPIO into MRL/lpr lupus mice resulted in a significant decrease in T2 relaxation times (from 93.3 ± 10.3 ms to 66.3 ± 6.4 ms; P < 0.008) in the inner medulla of the kidney at 24–48 h after injection. A smaller decrease in T2 relaxation times was observed in the outer medulla and cortex. No significant reduction was observed in the muscle, fat, or spleen of MRL/lpr lupus mice. No reduction of T2 relaxation times was detected in the kidneys of wild-type mice after injection of CR2-Fc-SPIO; in addition, no reduction of T2 relaxation times was detected in the kidneys of MRL/lpr lupus mice after injection of SPIO alone. Negative contrast was clearly visualized in the kidneys of MRL/lpr lupus mice but not in the kidneys of wild-type mice at 4–72 h after injection of CR2-Fc-SPIO. Histochemical staining of iron showed that CR2-Fc-SPIO nanoparticles were still detected in the glomeruli and tubules of MRL/lpr mice at 72 h after injection. No such staining was observed in the kidneys of normal mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CR2%20SPIO%20and%20human)]

No publication is currently available.

## NIH Support

DK076690, AI31105, P30 CA046934, T32 CA079446

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bao L., Quigg R.J. (2007). Complement in lupus nephritis: the good, the bad, and the unknown. Semin Nephrol.
3 Zhang X., Kohl J. (2010). A complex role for complement in allergic asthma. Expert Rev Clin Immunol.
4 Rovin B.H., McKinley A.M., Birmingham D.J. (2009). Can we personalize treatment for kidney diseases?. Clin J Am Soc Nephrol.
5 Kovacs, J.M., J.P. Hannan, E.Z. Eisenmesser, and V.M. Holers, Biophysical investigations of complement receptor 2 (CD21, CR2) ligand Interactions reveal amino acid contacts unique to each receptor-ligand pair. J Biol Chem, 2010
6 Serkova N.J., Renner B., Larsen B.A., Stoldt C.R., Hasebroock K.M., Bradshaw-Pierce E.L., Holers V.M., Thurman J.M. (2010). Renal inflammation: targeted iron oxide nanoparticles for molecular MR imaging in mice. Radiology.